# Galactosyl serum albumin-rhodamine green

Chemical name: | Galactosyl serum albumin-rhodamine green
Abbreviated name: | GSA-RhodG
Synonym:
Agent Category: | Polypeptide
Target: | β-D-galactose receptor
Target Category: | Receptor binding
Method of detection: | Optical fluorescence imaging
Source of signal: | Rhodamine green (RhodG)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=galactosyl+serum+albumin+and+rhodamine+green)]

Optical fluorescence imaging is increasingly used to study biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

On their cell surface, a variety of cancer cells express receptors (lectins) that bind to glycosylated proteins (3, 4). The β-D-galactose receptor binds and internalizes proteins that contain galactose sugar residues. Galactosyl serum albumin (GSA) was labeled with rhodamine green (RhodG) to study in vivo biodistribution of the tracer in tumor-bearing mice (5). RhodG is an optical fluorescence dye with an absorbance maximum at 502 nm and an emission maximum at 527 nm with a high extinction coefficient of 75,000 M^-1^cm^-1^. GSA-RhodG was found to have a high accumulation in a variety of human ovarian adenocarcinomas in nude mice (5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+synthesis)]

GSA, which contains 23 galactosamine residues, was incubated with RhodG-succinoimidyl ester for 15 min at room temperature (5). GSA-RhodG was isolated by column chromatography. There were ~3 RhodG molecules per GSA.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+and+in+vitro)]

Flow cytometry and fluorescent microscopy confirmed intracellular accumulation of GSA-RhodG to all nine human ovarian adenocarcinoma cell lines tested, with 89.5–99.8% of cells showing fluorescence (5). On the other hand, bovine serum albumin (BSA)-RhodG showed significantly lower intracellular accumulation with only 7.3–32.3% (P < 0.0001) of cells showing fluorescence. The mean fluorescence intensity for cells treated with GSA-RhodG (170.6) was >19-fold that of the cells treated with BSA-RhodG (8.6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+rodentia)]

Gunn et al. (5) performed biodistribution studies of GSA-RhodG in nude mice bearing intraperitoneal (i.p.) xenografts of human ovarian adenocarcinoma from the SHIN3, SKOV3, OVCAR5, or OVCAR8 cell lines. Images were obtained after i.p. injection of 25 μg (~0.3 nmol) of GSA-RhodG. Substantial fluorescence intensity was observed in all tumors formed from the four tumor cell lines in the exposed abdomen at 3 h after injection. Tumors <1 mm in diameter were visible. On the other hand, BSA-RhodG treatment revealed minimal tumor fluorescence. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Stockert R.J. (1995). The asialoglycoprotein receptor: relationships between structure, function, and expression. Physiol Rev.
4 Hama Y., Urano Y., Koyama Y., Choyke P.L., Kobayashi H. (2006). Targeted optical imaging of cancer cells using lectin-binding BODIPY conjugated avidin. Biochem Biophys Res Commun.
5 Gunn A.J., Hama Y., Koyama Y., Kohn E.C., Choyke P.L., Kobayashi H. (2007). Targeted optical fluorescence imaging of human ovarian adenocarcinoma using a galactosyl serum albumin-conjugated fluorophore. Cancer Sci.